# R-(−)-[^11^C]Epinephrine

Chemical name: | R-(–)-[^11^C]Epinephrine
Abbreviated name: | [^11^C]EPI
Synonym: | [^11^C]Epinephrine
Agent Category: | Compound
Target: | Norepinephrine transporter (NET), vesicular monoamine transporter (VMAT), neuronal storage vesicle, monoamine oxidase (MAO), catechol-O-methyltransferase (COMT)
Target Category: | Transporter binding, storage in sympathetic nervous system (SNS)
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Non-primate non-rodent mammals; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-Epinephrine%20OR%20%5B11C%5DEPI%20OR%20%5B11C%5DEpinephrine)]

R-(–)-[^11^C]Epinephrine ([^11^C]EPI) is a radioligand developed for positron emission tomography (PET) imaging of the sympathetic nervous system (SNS) (1, 2, 11). It is a catecholamine analog labeled with ^11^C, a positron emitter with a physical half-life (t_½_) of 20.4 min.

Many diseases affect the SNS, and imaging of pathologic changes of adrenergic transmission has been an important area of PET research (3, 4). Most postganglionic sympathetic neurons in the autonomic nervous system release the neurotransmitter norepinephrine (NE), which stimulates adrenergic receptors in various effector organs (5). There are different types and subtypes of adrenergic receptors, and they are characterized as α_1a_ to α_1c_, α_2a_ to α_2c_, and β_1_ to β_3_ (6). All of the NE receptors belong to the G-protein-linked receptor superfamily and mediate slow neuromodulatory postsynaptic responses. The NE transporter (NET) is a transmembrane protein located in the adrenergic nerve terminals that is responsible for active reuptake (uptake-1) of NE released from neurons (7). NE is stored in the neuronal vesicles and is released on stimulation. Significant expression of NET is found in major organs of the SNS, such as the heart and brain. There is substantial evidence that aberrations in cardiac SNS function contribute to the morbidity and mortality associated with cardiac diseases (8).

Molecular probes with structures closely related to NE can be used to assess the integrity of presynaptic sympathetic nerve terminals in various diseases. In vivo NE synthesis is similar to dopamine synthesis, and dopamine is converted to NE by the enzyme dopamine-β-hydroxylase (6). [^123^I]-meta-Iodobenzylguanidine ([^123^I]MIBG), a single-photon emission tomography (SPECT) agent, has been developed and used for neuronal imaging (9). Efforts have been made to develop a positron-emitting tracer because of the inadequate quantitative information and lower spatial resolution obtained by SPECT imaging with [^123^I]MIBG. EPI is a N-methyl derivative of (–)-norepinephrine and is produced in vivo together with NE by the adrenal medulla and other chromaffin tissues (6, 9, 10). EPI is handled in vivo in a manner similar to that for NE, with binding to NET and transport by vesicular monoamine transporter into neuronal vesicles for storage. EPI is subject to metabolism by both monoamine oxidase and catechol-O-methyltransferase. Langer and Halldin (9) have reviewed and compared various PET and SPECT tracers for mapping the cardiac nervous system.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-Epinephrine%20OR%20%5B11C%5DEPI%20OR%20%5B11C%5DEpinephrine%20AND%20synthesis)]

Soussain et al (1) first synthesized [^11^C]EPI by enzyme-catalyzed methylation. In that procedure, the [^11^C]methyl group was sequentially transferred from L-[methyl-^11^C]methionine to R-(–)-NE via S-adenosyl-L-[methyl-^11^C]methionine by the enzyme phenylethanolamine-N-methyl transferase. L-[methyl-^11^C]Methionine was first obtained by methylation of L-homocysteine thiolactone in a basic solution with [^11^C]methyl iodide in acetone. The reaction was completed in 28-31 min. L-[methyl-^11^C]Methionine was then enzymatically converted by L-methionine-S-adenosine transferase with adenosine triphosphate to S-adenosyl-L-[methyl-^11^C]methionine. This step was done by incubating the mixture for 12 min at 40 °C. The final yield was reported to be 20% (55.5 MBq (1.5 mCi) at 65 min at the end of bombardment (EOB)) in 30-35 min from [^11^C]methionine. The specific activity was 6.29 GBq (0.17 Ci)/μmol.

Chakraborty et al. (11) used a direct methylation method based on the fact that the parent amine was present in large excess, which minimized the probability of polymethylation. R-(–)-NE hydrochloride obtained commercially was first converted to free base by reaction with tetrabutylammonium hydrochloride under oxygen-free conditions. Either [^11^C]methyl iodide or [^11^C]methyl triflate was used as the radiomethylating agent. Free R-(–)-NE base was reacted with the methylating agent in dimethylformamide/dimethyl sulfoxide (3/1) and heated at 85 °C for 5 min. The product was purified by cation-exchange high-performance liquid chromatography. With [^11^C]methyl iodide, the radiochemical yield was 5-10% at the EOB in a synthesis time of 35-40 min. The specific activity was 37-74 GBq (1-2 Ci)/μmol. When [^11^C]methyl triflate was used, the yield was improved to 15-25% at the EOB with a specific activity of 33.3-81.4 GBq (0.9-2.2 Ci)/μmol

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-Epinephrine%20OR%20%5B11C%5DEPI%20OR%20%5B11C%5DEpinephrine%20AND%20in%20vitro)]

Soussain et al. (1) performed a specific binding study of [^11^C]EPI prepared by the enzymatic method in rat liver plasma membranes and found that the dissociation constant (K_D_) was 54 nM, as determined by Scatchard plot. The capacity of specific binding sites (B_max_) was 412 fmol/mg. In comparison, (–)-^3^H-NE had a K_D_ of 130 ± 60 nM and B_max_ of 340 ± 70 fmol/mg.

Nguyen et al. (12) conducted a myocardial kinetic study of [^11^C]EPI in an isolated working rat heart model. [^11^C]EPI was obtained with a specific activity of 18.5-37 GBq (0.5-1 Ci)/μmol and radiochemical purity >95%. All hearts were perfused with 11.1-16.7 MBq (300-450 μCi)/liter [^11^C]EPI in a buffer for 20 min followed by 20 min of wash-out. There were no significant differences in the hemodynamic data (heart rate, pressure, coronary flow, and cardiac output) between the treated group and the untreated control group. [^11^C]EPI had linear wash-in kinetics with K_i_ = 0.596 ± 0.198 ml/g/min and monoexponential wash-out kinetics with a clearance rate constant (k_2_) of 0.00121 ± 0.00114 min^–1^. The study indicated that the slow clearance during wash-out represented avid retention of [^11^C]EPI in the myocardium. The study also indicated that 61% of ^11^C]EPI was metabolized and released. [^11^C]EPI radioactivity uptake and retention was decreased by treatment with 50 nM desipramine (DMI), an uptake-1 inhibitor, for both the wash-in and wash-out periods. When DMI was added to the wash-out period only, no effect was observed, indicating that the retention was independent of uptake-1 activity. Treatment with reserpine (vesicular blocker) decreased the K_i_ to 0.034 ± 0.010 ml/g/min and increased k_2_ to 31.02 ± 10.88 min^–1^.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C-Epinephrine%20OR%20%5B11C%5DEPI%20OR%20%5B11C%5DEpinephrine%29%20AND%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C-Epinephrine%20OR%20%5B11C%5DEPI%20OR%20%5B11C%5DEpinephrine%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

Soussain et al. (1) injected 8.14 MBq (0.22 mCi) of enzyme-prepared [^11^C]EPI into a rabbit and studied the tissue distribution by gamma imaging and blood kinetics by serial blood samples. The images showed that the distribution was mainly in the heart, liver-pancreas, kidneys, suprarenal glands, and urinary bladder. The brain was not imaged. The blood kinetic study estimated that the global biologic t_½_ in the circulating blood was 3 min.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C-Epinephrine%20OR%20%5B11C%5DEPI%20OR%20%5B11C%5DEpinephrine%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C-Epinephrine%20OR%20%5B11C%5DEPI%20OR%20%5B11C%5DEpinephrine%29%20AND%20human)]

Munch et al. (2) evaluated [^11^C]EPI and [^11^C]meta-hydroxyephedrine ([^11^C]mHED) in 7 healthy volunteers and in 10 patients who had undergone heart transplantation within the previous 3.5-48 months. The specific activity, radiochemical purity, and chemical purity of the [^11^C]EPI used were 33.3-74 GBq (0.9-2 Ci)/μmol, 98%, and 97%, respectively. The volunteers and patients received [^11^C]EPI doses of 466.2 ± 29.6 MBq (12.6 ± 0.8 mCi) and 514.3 ± 44.4 MBq (13.9 ± 1.2 mCi), respectively. Blood sample analysis showed that [^11^C]EPI was rapidly metabolized in both volunteers and patients. Unmetabolized [^11^C]EPI in the blood was 65% at 5 min and decreased to <20% and 14% after 20 and 60 min, respectively. Clearance of activity from the myocardium was much slower; the myocardium clearance t_½_ was 10.5 ± 3.2 h in healthy volunteers and 4.0 ± 1.1 in transplant patients. In comparison, the myocardium clearance t_½_ of [^11^C]mHED was 4.3 ± 2.4 and 1.5 ± 0.2 h, respectively. Images showed high myocardial uptake of [^11^C]EPI radioactivity in volunteers and greatly reduced activity (up to 80% in denervated areas) in transplant patients. At 35 min in volunteers, the metabolite-corrected mean myocardial retention for [^11^C]EPI was significantly greater than for [^11^C]mHED (0.295 ± 0.022 min^–1^versus 0.142 ± 0.012 min^–1^; P < 0.0001). These values were significantly lower (P < 0.0001) in transplant patients: 0.055 ± 0.004 min^–1^ and 0.050 ± 0.006 min−^1^ for [^11^C]EPI and [^11^C]mHED, respectively.

## NIH Support

NIH R01 H641047-01, R01 HL27555-06.

## References

1 Soussain R., Gueguen P., Morgat J.L., Maziere M., Berger G., Comar D. (1984). Enzymatic-synthesis of C-11-labelled (-)-epinephrine. Journal of Labelled Compounds & Radiopharmaceuticals.
2 Munch G., Nguyen N.T., Nekolla S., Ziegler S., Muzik O., Chakraborty P., Wieland D.M., Schwaiger M. (2000). Evaluation of sympathetic nerve terminals with [(11)C]epinephrine and [(11)C]hydroxyephedrine and positron emission tomography. Circulation.
3 Konishi, J., B.A. Dwamena, M.D. Gross, B. Shapiro, T. Misaki, M. Fukunaga, J.C. Sisson, H.-Y. Oei, M. De Jong, and E. P. Krenning Endocrinology, in Molecular Nuclear Medicine, L.E. Feinendegen, W.W. Shreeve, W.C. Eckelman, Y.-W. Bahk, and H.N. Wagner Jr., Editor. 2003, Springer: New York. p. 357-409.
4 Antoni, G., T. Kihlberg, and B. Langstrom, Aspects on the synthesis of 11C-Labelled compounds, in Handbook of Radiopharmaceuticals, M.J. Welch, and C.S. Redvanly, Editor. 2003, John Wiley & Sons Ltd.: West Sussex, England. p. 141-194.
5 Sunderland, P.M., Pathophysiology. The Biologic basis for disease in adults and children, K.L. McCance, and S. E. Huether, Editor. 1994, Mosby-Year Books, Inc.: St, Louiis. p. 397-436.
6 Frey, K.A., PET study of neurochemical systems, in Positron Emission Tomography, P.E. Valk, D.L. Bailey, D.W. Townsend, and M.N. Maisey, Editors. 2002, Springer London. p. 309-327.
7 Buursma A.R., Beerens A.M., de Vries E.F., van Waarde A., Rots M.G., Hospers G.A., Vaalburg W., Haisma H.J. (2005). The Human Norepinephrine Transporter in Combination with 11C-m-Hydroxyephedrine as a Reporter Gene/Reporter Probe for PET of Gene Therapy. J Nucl Med.
8 Caldwell J.H., Kroll K., Li Z., Seymour K., Link J.M., Krohn K.A. (1998). Quantitation of presynaptic cardiac sympathetic function with carbon-11-meta-hydroxyephedrine. J Nucl Med.
9 Langer O., Halldin C. (2002). PET and SPET tracers for mapping the cardiac nervous system. Eur J Nucl Med Mol Imaging.
10 Antoni, G., T. Kihlberg, and B. Langstrom, Aspects on the synthesis of 11C-labelled compounds, in Handbook of radiopharmaceuticals, M.J. Welch and C.S. Redvanly, Editors. 2003, John Wiley & Sons Ltd: Chichester. p. 141-194.
11 Chakraborty P.K., Gildersleeve D.L., Jewett D.M., Toorongian S.A., Kilbourn M.R., Schwaiger M., Wieland D.M. (1993). High yield synthesis of high specific activity R-(-)-[11C]epinephrine for routine PET studies in humans. Nucl Med Biol.
12 Nguyen N.T., DeGrado T.R., Chakraborty P., Wieland D.M., Schwaiger M. (1997). Myocardial kinetics of carbon-11-epinephrine in the isolated working rat heart. J Nucl Med.